# FluidMAG iron nanoparticle-labeled mesenchymal stem cells for tracking cell homing to tumors

Chemical name: | FluidMAG iron nanoparticle-labeled mesenchymal stem cells for tracking cell homing to tumors
Abbreviated name: | FluidMAG iron nanoparticle-labeled MSCs
Synonym: | Iron-labeled MSCs
Agent Category: | Cells
Target: | Others (cell imaging)
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=mesenchymal+stem+cells+and+cell+tracking+and+imaging)]

Personalized diagnosis and treatment with allogenic or autologous cells are becoming a reality in the field of medicine (1, 2). Cytotoxic or engineered T-cells (http://clinicaltrials.gov/ct2/results?term=cytotoxic+T+cells) are under clinical trial for the treatment of hematopoietic or other malignant diseases (3). Contrast agent–tagged macrophages (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging) are used as cellular probes to image the early inflammatory processes in macrophage-rich conditions such as inflammation, atherosclerosis, and acute cardiac graft rejection (4). The roles of stem cells (http://clinicaltrials.gov/ct2/results?term=stem+cell) are under intensive investigation in therapeutic and regenerative medicine, such as regenerating cardiomyocytes, neurons, bone, and cartilage (1). Genetically modified cells (http://clinicaltrials.gov/ct2/results?term=genetic+disorders+and+cells) are used to treat genetic disorders (5). With promising results from these studies, a critical issue is how to monitor the temporal and spatial migration and the homing of these cells, as well as the engraftment efficiency and functional capability of the transplanted cells in vivo (6, 7). Histopathological techniques have only been used to obtain information on the fate of implanted cells at the time of animal euthanization or via biopsy or surgery. To track the real-time changes of cell location, viability, and functional status, cell imaging techniques have been introduced during the last few years. Cells of interest are labeled with reporter genes, fluorescent dyes, or other contrast agents that transform the tagged cells into cellular probes or imaging agents (2, 6, 7).

The ability to monitor superparamagnetic iron oxide particles (SPIO) with magnetic resonance imaging (MRI) has been utilized in animal models as well as in a few clinical settings to investigate the fate of labeled cells (6-10). The advantages of using MRI for cell tracking include the high spatial resolution with high anatomic background contrast, the lack of exposure to ionizing radiation, and the ability to follow the cells for months, although it is difficult to measure the rate of cell division and to determine whether each progeny shares the SPIO in vivo. In addition, cell labeling with SPIO nanoparticles is generally nontoxic and does not affect the cell proliferation and differentiation capacity, although a few studies have reported that the stem cells labeled with SPIO lose part of their differentiation capacity in a SPIO concentration–dependent manner. An important limitation of MRI is the fact that MRI signals cannot indicate whether cells are dead or alive. It is also unknown whether the MRI signal comes from targeted or labeled cells or from macrophages. Basically, SPIO particles are used to label the target cells by systemic application or by injection into the tissue area of interest to monitor target cell migration after phagocytosis. SPIO are more frequently used to label the cells in vitro by incorporating into the cells directly. Furthermore, SPIO are usually encapsulated by organic polymers to increase their stability and biocompatibility and to allow the chemical modification of their surfaces. The fact is that the uptake of different particles varies largely between different cell types and between particle coatings (6, 7).

Msenchymal stem cells (MSCs) represent a heterogeneous subset of pluripotent stromal cells that can be isolated from different adult tissues including adipose tissue, liver, muscle, amniotic fluid, placenta, umbilical cord blood, and dental pulp, although the bone marrow remains the principal source for most preclinical and clinical studies (1, 11, 12). Although MSCs account for only 0.001–0.01% of the total nucleated cells within isolated bone marrow aspirates, they can easily be isolated and expanded in vitro through as many as 40 population doublings after 8–10 weeks of culture (1, 13). These cells exhibit the potential to differentiate into cells of diverse lineages such as adipocytes, chondrocytes, osteocytes, myoblasts, cardiomyocytes, neurons, and astrocytes. In addition, MSCs show tropism or homing to tumors and thus have been used as vehicles for directed cancer delivery (14, 15). The mechanism responsible for the homing of MSCs to tumors is thought to involve chemokine ligands and receptors, as with the recruitment of leukocytes to areas of inflammation. However, unlike with leukocytes, the specific chemokines responsible for MSC migration are poorly characterized (14, 15). Nevertheless, homing to tumors has been confirmed with traditional immunohistochemistry and other methods in many studies. Loebinger et al. labeled MSCs with fluidMAG iron nanoparticles and imaged homing of the labeled MSCs to tumors with MRI (16). FluidMAG nanoparticles are commercially available ferrofluids consisting of an aqueous dispersion of magnetic iron oxides with a hydrodynamic diameter of 200 nm and a starch coating. The investigators showed that as few as 1,000 labeled MSCs were detected 1 month after their co-injection with breast cancer cells that formed subcutaneous tumors. The investigators further demonstrated that intravenously injected labeled cells could be tracked in vivo to home to multiple lung metastases (16).

### Relevant Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cell+tracking+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Mesenchymal stem cells under clinical trails (http://clinicaltrials.gov/ct2/results?term=mesenchymal+stem+cells)
- SPIO and cell imaging under clinical trails (http://clinicaltrials.gov/ct2/results?term=SPIO+and+cell+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19920196?ordinalpos=&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.SmartSearch&log$=citationsensor)]

Loebinger et al. labeled human adult MSCs with fluidMAG iron nanoparticles through overnight incubation with the nanoparticles in cell culture medium (0.5 mg/ml) (16). FluidMAG nanoparticles are commercially available ferrofluids consisting of an aqueous dispersion of magnetic iron oxides with a hydrodynamic diameter of 200 nm and a starch coating. The cells were then vigorously washed with phosphate-buffered saline to remove any free particles. Internalization of the nanoparticles into MSCs was confirmed with Prussian blue staining, electron microscopy, and confocal microscopy. The labeled cells contained up to 30 pg iron oxide per MSC. The percentage of labeled cells in total (labeling efficiency) was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19920196?ordinalpos=&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.SmartSearch&log$=citationsensor)]

Loebinger et al. analyzed the effect of labeling on the properties of MSCs with different techniques (16). Their analysis showed that the labeled cells retained their MSC characteristics and the ability to differentiate into stromal tissues, including bone and fat (data not shown). The labeled and unlabeled MSCs had equivalent in vitro tumor homing (104.4 ± 5.6 versus 113.1 ± 16.1 cells per ×10 magnification field; P > 0.05) in transwell migration studies. There was no effect of iron nanoparticles on MSC proliferation, as shown by MTS NAD(P)H-dependent proliferation assay, or on cell viability, as shown by annexin V flow cytometry apoptosis assay (33.0 ± 4.2% versus 29.4 ± 2.1% dead or apoptotic cells without and with labeling; P > 0.05). It is unclear whether all these studies depend on the cells labeled with fluidMAG or a mixture of labeled and unlabeled cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19920196?ordinalpos=&itool=EntrezSystem2.PEntrez.Pubmed.Pubmed_ResultsPanel.SmartSearch&log$=citationsensor)]

Loebinger et al. first evaluated the sensitivity of MRI by assessing the dose response of iron-labeled cells in subcutaneous tumor xenografts (16). For this purpose, the investigators double-labeled the MSCs with fluorescent dye Dil and fluidMAG iron nanoparticles, and they then injected MDAMB231 human breast cancer cells (2 × 10^6^) subcutaneously with increasing numbers of labeled MSCs in nonobese diabetic/severe combined immunodeficient mice (n = 2 mice/group). Using a 9.4-T MRI system, Loebinger et al. were able to visualize as few as 1,000 labeled MSCs in tumors 28 days after injection. Signal voids were not visible at 28 days when unlabeled MSCs, dead labeled MSCs, or free iron were co-administered with the tumor cells. Histopathological examination confirmed the presence of the iron nanoparticles only in the tumors injected with live labeled MSCs. This was further confirmed with co-localization of the Prussian blue staining of iron and DiI fluorescence within the MSCs.

Loebinger et al. then tracked cell homing in a pulmonary metastasis animal model (16). The model was established by injection of 2 × 10^6^ MDAMB231 cells into the tail vein. The investigators were able to detect lung metastases, which were visualized as diffuse hyperintensities in all five lobes 38 days after tumor cell injection, using MRI without contrast agents. Therefore, 35 days after intravenous delivery of MDAMB231 cells, Loebinger et al. injected MSCs double-labeled with DiI and iron nanoparticles intravenously. MRI imaging at 1 h and 24 h after the MSC injection showed a decrease in signal intensity in the metastatic lesions, indicating that the iron-labeled MSCs homed into these tumors (n = 4 mice). The signal/noise ratio was significantly decreased across all four radiological areas, as compared with ratios before MSC injection (n = 3 mice, P = 0.005). Immunohistochemistry confirmed that DiI/Fe-stained cells were within or adjacent to tumors, and the labeled cells were not macrophages.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Mathiasen A.B., Haack-Sorensen M., Kastrup J. (2009). Mesenchymal stromal cells for cardiovascular repair: current status and future challenges. Future Cardiol.
2 Arbab A.S., Janic B., Haller J., Pawelczyk E., Liu W., Frank J.A. (2009). In Vivo Cellular Imaging for Translational Medical Research. Curr Med Imaging Rev.
3 Cesco-Gaspere M., Morris E., Stauss H.J. (2009). Immunomodulation in the treatment of haematological malignancies. Clin Exp Med.
4 Eisenblatter M., Ehrchen J., Varga G., Sunderkotter C., Heindel W., Roth J., Bremer C., Wall A. (2009). In vivo optical imaging of cellular inflammatory response in granuloma formation using fluorescence-labeled macrophages. J Nucl Med.
5 Bachoud-Levi A.C. (2009). Neural grafts in Huntington's disease: viability after 10 years. Lancet Neurol.
6 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
7 Hoehn M., Wiedermann D., Justicia C., Ramos-Cabrer P., Kruttwig K., Farr T., Himmelreich U. (2007). Cell tracking using magnetic resonance imaging. J Physiol.
8 Park, K.S., J. Tae, B. Choi, Y.S. Kim, C. Moon, S.H. Kim, H.S. Lee, J. Kim, J.S. Kim, J. Park, J.H. Lee, J.E. Lee, J.W. Joh, and S. Kim, Characterization, in vitro cytotoxicity assessment, and in vivo visualization of multimodal, RITC-labeled, silica-coated magnetic nanoparticles for labeling human cord blood-derived mesenchymal stem cells. Nanomedicine, 2010
9 Wang H.H., Wang Y.X., Leung K.C., Au D.W., Xuan S., Chak C.P., Lee S.K., Sheng H., Zhang G., Qin L., Griffith J.F., Ahuja A.T. (2009). Durable mesenchymal stem cell labelling by using polyhedral superparamagnetic iron oxide nanoparticles. Chemistry.
10 Yoon T.J., Kim J.S., Kim B.G., Yu K.N., Cho M.H., Lee J.K. (2005). Multifunctional nanoparticles possessing a "magnetic motor effect" for drug or gene delivery. Angew Chem Int Ed Engl.
11 Ehrchen J., Helming L., Varga G., Pasche B., Loser K., Gunzer M., Sunderkotter C., Sorg C., Roth J., Lengeling A. (2007). Vitamin D receptor signaling contributes to susceptibility to infection with Leishmania major. FASEB J.
12 Sadan O., Melamed E., Offen D. (2009). Bone-marrow-derived mesenchymal stem cell therapy for neurodegenerative diseases. Expert Opin Biol Ther.
13 Huang D.M., Hsiao J.K., Chen Y.C., Chien L.Y., Yao M., Chen Y.K., Ko B.S., Hsu S.C., Tai L.A., Cheng H.Y., Wang S.W., Yang C.S. (2009). The promotion of human mesenchymal stem cell proliferation by superparamagnetic iron oxide nanoparticles. Biomaterials.
14 Kuhn N.Z., Tuan R.S. (2010). Regulation of stemness and stem cell niche of mesenchymal stem cells: implications in tumorigenesis and metastasis. J Cell Physiol.
15 Feng B., Chen L. (2009). Review of mesenchymal stem cells and tumors: executioner or coconspirator?. Cancer Biother Radiopharm.
16 Loebinger M.R., Kyrtatos P.G., Turmaine M., Price A.N., Pankhurst Q., Lythgoe M.F., Janes S.M. (2009). Magnetic resonance imaging of mesenchymal stem cells homing to pulmonary metastases using biocompatible magnetic nanoparticles. Cancer Res.